# (E)-2-(2-(2-(2-[^18^F]Fluoroethoxy)ethoxy)ethoxy)-5-(4-dimethylaminostyryl)-pyridine

Chemical name: | (E)-2-(2-(2-(2-[^18^F]Fluoroethoxy)ethoxy)ethoxy)-5-(4-dimethylaminostyryl)-pyridine
Abbreviated name: | [^18^F]FPEGN3-Styrylpyridine, [^18^F]2
Synonym:
Agent category: | Compound
Target: | Amyloid-beta peptide
Target category: | Acceptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation:
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Styrylpyridine)]

Alzheimer's disease (AD) is a form of dementia with a gradual memory loss and a progressive decline in mental functions with time (1, 2). It is characterized pathologically by neuronal loss, extracellular amyloid-beta senile plaques (APs; aggregates of amyloid-beta peptides consisting of 40 to 42 amino acids) and intracellular neurofibrillary tangles (NFTs; filaments of microtubule-binding hyper-phosphorylated protein tau) in the brain, especially in the hippocampus and associative regions of the cortex (3, 4). Beta-amyloid peptides and tau protein are implicated as the main causes of neuronal degeneration and cell death (5, 6).

Early diagnosis of AD is important for treatment consideration and disease management (7). Various amyloid imaging agents have been developed for MRI, SPECT, and PET (8-13). The binding of different derivatives of Congo red, thioflavin, stibene, and aminonaphthalene has been studied in human post-mortem brain tissue and in transgenic mice. Out of these analogues, 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malono nitrile ([^18^F]FDDNP (http://www.ncbi.nlm.nih.gov/books/NBK23038/)) was first studied in humans, showing more binding in the brains of patients with AD than in those of healthy people (14). Despite of its slow clearance kinetics for PET imaging, [^18^F]FDDNP has been found to be a useful tool for detection of both NFTs and APs in AD patients. [^11^C]PIB (http://www.ncbi.nlm.nih.gov/books/NBK23443/), also known as Pittsburgh Compound B or [^11^C]6-OH-BTA-1, showed marked retention in brain cortices known to contain substantial amounts of APs. Other radioligands tested in humans were [^11^C]4-N-methylamino-4´-hydroxystilbene ([^11^C]SB-13 (http://www.ncbi.nlm.nih.gov/books/NBK23321/), a stilbene derivative), and [^125^]IMPY (http://www.ncbi.nlm.nih.gov/books/NBK23612/) (a pyridine derivative), which displayed a high accumulation in the frontal cortex in AD patients. (E)-2-(2-(2-(2-[^18^F]Fluoroethoxy)ethoxy)ethoxy)-5-(4-dimethylaminostyryl)-pyridine ([^18^F]FPEGN3-styrylpyridine) is a modified stilbene derivative, in which one of the benzene rings of stilbene was replaced with one pyridine ring (15). [^18^F]FPEGN3-styrylpyridine is being developed as a PET for amyloid plaque imaging.

### Related Resource Links:

- Chapters in MICAD (Amyloid (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Amyloid (http://www.ncbi.nlm.nih.gov/gene/351))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amyloid (http://www.ncbi.nlm.nih.gov/omim/?term=Amyloid))
- Clinical trials (Amyloid (http://www.clinicaltrials.gov/ct2/results?term=Amyloid))
- Drug information in FDA (Amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Styrylpyridine%20and%20synthesis)]

Zhang et al. (15) prepared [^18^F]FPEGN3-styrylpyridine by [^18^F]fluoride nucleophilic displacement of the corresponding tosylate precursor in the presence of Kryptofix 2.2.2/K_2_CO_3_ with a high labeling yield (49-53%, decay-corrected) and a high radiochemical purity (>99%). Specific activity at the end of synthesis (50 min) was determined to be 41-54 GBq/mmol (1,500-2,000 Ci/mmol). [^18^F]FPEGN3-styrylpyridine showed adequate lipophilicity (log P = 3.22) for crossing the blood-brain barrier.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Styrylpyridine%20and%20in%20vitro)]

FPEGN3-styrylpyridine was reported to have high binding affinity (K_i_ = 2.5 ± 0.4) for β-amyloid plaques in homogenates of postmortem human AD brain membranes, using [^125^]IMPY as the radioligand (15). The binding affinity is similar to SB-13 (K_i_ = 1.2 ± 0.7) as previously reported (10). Furthermore, 8-10 fold higher specific binding of [^18^F]FPEGN3-styrylpyridine was detected in the gray matter than in white matter homogenates of AD brains, where β-amyloid plaques were low or nonexistent. The binding of [^18^F]FPEGN3-styrylpyridine to both gray and white matter from normal control brains was also low. In vitro autoradiography confirmed the binding of [^18^F]FPEGN3-styrylpyridine to discrete regions in the gray matter and not to the while matter of AD brain sections.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Styrylpyridine%20and%20rodentia)]

[^18^F]FPEGN3-styrylpyridine (0.19-0.37 MBq, 5-10 μCi) was injected intravenously into normal mice (n = 3) to study its accumulation into the brain and other organs (15). The radioactivity in the excised brain samples was measured at 2, 30, 60 and 120 min after injection. [^18^F]FPEGN3-styrylpyridine showed a good accumulation in the brain with 7.77% ID/g at 2 min, 1.03% ID/g at 30 min, 1.28% ID/g at 60 min and 0.84% ID/g at 120 min. The liver and kidneys exhibited higher radioactivity accumulation than the brain at all time points. The radioactivity in the bone was 1.64% ID/g at 120 min, suggesting defluorination in mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Styrylpyridine%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Styrylpyridine%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Styrylpyridine%20and%20human)]

No publication is currently available.

## NIH Support

AG022559, AG21868

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci.
3 Hardy J.A., Higgins G.A. (1992). Alzheimer's disease: the amyloid cascade hypothesis. Science.
4 Mirra S.S., Heyman A., McKeel D., Sumi S.M., Crain B.J., Brownlee L.M., Vogel F.S., Hughes J.P., van Belle G., Berg L. (1991). Part II. Standardization of the neuropathologic assessment of Alzheimer's disease. Neurology.
5 Brandt R., Hundelt M., Shahani N. (2005). Tau alteration and neuronal degeneration in tauopathies: mechanisms and models. Biochim Biophys Acta.
6 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
7 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
8 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
9 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
10 Kung M.P., Hou C., Zhuang Z.P., Skovronsky D., Kung H.F. (2004). Binding of two potential imaging agents targeting amyloid plaques in postmortem brain tissues of patients with Alzheimer's disease. Brain Res.
11 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
12 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
13 Verhoeff N.P., Wilson A.A., Takeshita S., Trop L., Hussey D., Singh K., Kung H.F., Kung M.P., Houle S. (2004). In-vivo imaging of Alzheimer disease beta-amyloid with [11C]SB-13 PET. Am J Geriatr Psychiatry.
14 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
15 Zhang W., Kung M.P., Oya S., Hou C., Kung H.F. (2007). (18)F-labeled styrylpyridines as PET agents for amyloid plaque imaging. Nucl Med Biol.